# ^64^Cu-Labeled 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar) conjugated to cyclic arginine-glycine-aspartic acid (RGD) peptide

Chemical name: | ^64^Cu-Labeled 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar) conjugated to cyclic arginine-glycine-aspartic acid (RGD) peptide
Abbreviated name: | [^64^Cu]-AmBaSar-RGD
Synonym:
Agent Category: | Compound
Target: | α_v_β_3_ integrin
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^64^Cu]-AmBaSar-RGD for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=AmBaSar&cmd=DetailsSearch)]

The integrin α_v_β_3_ receptor is one of several known biomarkers of cancerous tumor angiogenesis (1) and metastasis (2). Therefore, molecular imaging (MI) of integrin α_v_β_3_ receptor expression in tumors is considered to be useful for the detection of malignant tumors and the development of an individualized treatment and monitoring regimen for the patient (3). Ligands such as vitronectin, fibronectin, etc., which interact with integrins, are known to bind these receptors through an Arg-Gly-Asp (RGD) epitope. Consequently, many MI probes used for the detection and quantification of integrins with positron emission tomography (PET) or multimodal imaging are based on an RGD motif containing a peptide or its derivative and are labeled with ^18^F or are conjugated to a chelator for the binding of ^64^Cu (3, 4). In this regard, ^64^Cu can be considered to be a more suitable nuclide than ^18^F (half-life, ~110 min) for the development of a MI probe that can be used to detect integrin α_v_β_3_ receptors because of its longer half-life (12.7 h) because a longer circulation time can be necessary for the penetration of dense tumors (5). Recently a cage-like bifunctional chelator, 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo [6.6.6] icosane-1-ylamino)methyl)benzoic acid (AmBaSar) was developed and conjugated to RGD for labeling with ^64^Cu ([^64^Cu]-AmBaSar-RGD) (3). Subsequently, Cai et al. evaluated the biodistribution of [^64^Cu]-AmBaSar-RGD and its effectiveness in the detection of tumors expressing integrin α_v_β_3_ receptors in mice bearing U-87MG cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-14&Template=cellBiology) tumors, which express integrin α_v_β_3_ receptors (3).

### Other Sources of Information

- Chapters on integrins in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=integrins+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001144999.1) of human alpha v isoforms 2 integrin
- Articles about integrins in Online Mendelian Inheritance in Man Database (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=integrins)
- Integrin clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=integrins)
- Integrin related pathways in Pathways Interaction Database (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=integrin)
- Natalizumab – an alpha(4)beta(1)-integrin antagonist [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=natalizumab%20review&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20synthesis&cmd=DetailsSearch)]

The synthesis of AmBaSar-RGD and its labeling with ^64^Cu have been described by Cai et al. (3). The radiochemical yield of the labeled compound was >95% with a purity of >99% as determined with high-performance liquid chromatography (HPLC). During radiographic thin-layer chromatography (radio-TLC) analysis, ^64^Cu remained at the origin and the R_f_ value of [^64^Cu]-AmBaSar-RGD was between 0.8 and 1.0 (3). The specific activity of the radiochemical was reported to be 10.1–22.2 GBq/μmol (272.7–599.4 mCi/μmol).

For comparison purposes, ^64^Cu-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) conjugated to RGD ([^64^Cu]-DOTA-RGD) was used in some studies (3). The radiochemical yield, purity, and specific activity of this radiocompound were 80%, 98%, and 10.1–22.2 GBq/μmol (272.7–599.4 mCi/μmol), respectively. The R_f_ value of [^64^Cu]-DOTA-RGD on radio-TLC analysis was reported to be between 0.8 and 1.0.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20in%20vitro&cmd=DetailsSearch)]

When [^64^Cu]-AmBaSar-RGD and [^64^Cu]-DOTA-RGD were respectively exposed to phosphate-buffered saline (pH 7.4), fetal bovine, or mouse serum, the stability of both tracers was reported to be >95% for up to 24 h as determined with HPLC (3).

The 1-octanol/water partition coefficients of [^64^Cu]-AmBaSar-RGD and [^64^Cu]-DOTA-RGD were reported to be −2.44 ± 0.12 and −2.80 ± 0.04, respectively, indicating that the two radiochemicals had a hydrophilic nature (3).

In a ^125^I-Labeled eschistatin binding assay (125I-eschistatin binds specifically to integrin α_v_β_3_ receptors) using U-87MG cells, the cellular binding of the ^125^I-labeled compound was shown to be inhibited by AmBaSar-RGD and c(RGDyK) (a derivative of RGD) in a dose-dependent fashion (3). The 50% inhibition concentration values of AmBaSar-RGD and c(RGDyK) were determined to be 53.26 ± 0.51 nmol/L and 36.55 ± 0.65 nmol/L, respectively.

In another study, both [^64^Cu]-AmBaSar-RGD and [^64^Cu]-DOTA-RGD were shown to bind the U-87MG cells and only 0.1%–0.4% of the radiochemicals was internalized by the cells (3). In addition, the cellular binding of both tracers was shown to be blocked by an excess amount of unlabeled c(RGDyK) (2 μg).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20rodentia&cmd=DetailsSearch)]

The metabolic stability of [^64^Cu]-AmBaSar-RGD and [^64^Cu]-DOTA-RGD was evaluated in an athymic nude mouse bearing a U-87MG cell tumor as described by Cai et al. (3). The animal was administered either [^64^Cu]-AmBaSar-RGD or [^64^Cu]-DOTA-RGD through the intravenous route and euthanized 1 h later for the collection of blood and to obtain the liver, kidneys, and tumors from the animals. Subsequently, the blood and the kidney, liver, and tumor homogenate extracts were prepared and analyzed for uptake of the two radiochemicals with HPLC as detailed elsewhere (3). The amount of intact tracer in the blood, tumor, liver, and kidneys was reported to be 88%, 95%, 98%, and 98%, respectively, for [^64^Cu]-AmBaSar-RGD and 38%, 87%, 34%, and 74%, respectively, for [^64^Cu]-DOTA-RGD. This study indicated that [^64^Cu]-AmBaSar-RGD was more stable than [^64^Cu]-DOTA-RGD under in vivo conditions.

For the biodistribution study, nude mice bearing U-87MG cell tumors (n = 3/time point) were injected with the two tracers respectively and euthanized 20 h later to harvest all the major organs and determine the amount of radioactivity incorporated in the organs (3). Results obtained from this study were presented as percent injected dose per gram tissue (% ID/g), and the tumor/tissue ratios for the various organs were also calculated. At 20 h postinjection (p.i.), both tracers were shown to accumulate primarily in the kidneys, liver, stomach, intestine, and the tumors. With [^64^Cu]-AmBaSar-RGD, the uptake of radioactivity in the liver and kidneys was 0.55 ± 0.06% ID/g and 1.51 ± 0.27% ID/g, respectively, and for [^64^Cu]-DOTA-RGD the uptake in the liver and kidneys was 2.16 ± 0.85% ID/g and 0.98 ± 0.40% ID/g, respectively. For [^64^Cu]-AmBaSar-RGD, the tumor/muscle, tumor/heart, tumor/lung, tumor/liver, and tumor/kidney uptake ratios were 14.20 ± 3.84, 7.33 ± 1.55, 3.34 ± 0.70, 1.18 ± 0.05, and 0.43 ± 0.06, respectively. These ratios were 5.97 ± 2.25, 1.78 ± 0.37, 1.27 ± 0.37, 0.33 ± 0.09, and 0.66 ± 0.04, respectively, for [^64^Cu]-DOTA-RGD. This study indicated that both tracers had a similar uptake trend in the tissues of the animals.

In another study, the animals (n = 3 mice/tracer) were injected with either [^64^Cu]-AmBaSar-RGD or [^64^Cu]-DOTA-RGD in the presence of excess c(RGDyK) (10 mg/kg body weight), and the mice were euthanized 2 h later to determine the amount of radioactivity accumulated in the tumors and the major organ tissues (3). Control mice were injected with the radiochemicals alone and treated as the test animals. A significantly lower (P < 0.05) amount of radioactivity (0.09 ± 0.03% ID/g) accumulated in the tumors of animals co-injected with [^64^Cu]-AmBaSar-RGD and c(RGDyK) compared to tumors of control mice (1.85 ± 0.16% ID/g). A similar trend was noticed with [^64^Cu]-DOTA-RGD. This study indicated that [^64^Cu]-AmBaSar-RGD bound specifically to the integrin α_v_β_3_ receptors.

Static microPET scans were performed on nude mice bearing U-87MG cell tumors at 1, 2, 4, and 20 h after injection of [^64^Cu]-AmBaSar-RGD or [^64^Cu]-DOTA-RGD (n = 3 animals/time point) to determine the biodistribution pattern and tumor-targeting specificity of the tracers in the animals (3). From the PET images it was evident that both tracers accumulated in the tumors to a comparable extent at all time points; however, the biodistribution patterns of the two radiochemicals in the animals were significantly different from each other, especially in the liver and kidneys. The renal uptake of [^64^Cu]-AmBaSar-RGD reduced from 2.83 ± 0.77% ID/g at 1 h p.i. to 1.43 ± 0.35% ID/g at 20 h p.i., and for [^64^Cu]-DOTA-RGD the accumulation was 1.52 ± 0.46% ID/g at 1 h p.i. and showed only a slight change at 20 h p.i. (1.58 ± 0.13% ID/g). In general, the accumulation of [^64^Cu]-AmBaSar-RGD in the kidneys was higher than that of [^64^Cu]-DOTA-RGD from 1–4 h, and both tracers showed comparable levels of residual label in these organs at 20 h p.i. In the liver, the uptake of [^64^Cu]-AmBaSar-RGD was 0.89 ± 0.13% ID/g at 1 h p.i. and decreased to 0.64 ± 0.06% ID/g by 20 h p.i. The uptake of [^64^Cu]-DOTA-RGD in the liver was 2.28 ± 1.08% ID/g at 1 h p.i. and increased slightly to 2.52 ± 1.43% ID/g at 20 h p.i. The investigators noted that the uptake of [^64^Cu]-DOTA-RGD in the liver was significantly higher (P value not reported) than that of [^64^Cu]-AmBaSar-RGD at all time points.

MicroPET scans of mice (n = 3 animals/tracer) bearing U-87MG cell tumors injected with either [^64^Cu]-AmBaSar-RGD or [^64^Cu]-DOTA-RGD in the presence of a blocking dose of c(RDGyK) showed an almost complete elimination of tracer uptake by the tumors (3). This study confirmed the earlier observations made during the blocking study (described above) that [^64^Cu]-AmBaSar-RGD specifically bound the integrin α_v_β_3_ receptors.

From these studies, the investigators concluded that [^64^Cu]-AmBaSar-RGD had excellent metabolic stability and favorable in vivo pharmacokinetics for the PET detection of tumors expressing integrin α_v_β_3_ receptors (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20Non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20Non-human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-AmBaSar-RGD%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Dijkgraaf I., Boerman O.C. (2009). Radionuclide imaging of tumor angiogenesis. Cancer Biother Radiopharm.
2 Desgrosellier J.S., Cheresh D.A. (2010). Integrins in cancer: biological implications and therapeutic opportunities. Nat Rev Cancer.
3 Cai H., Li Z., Huang C.W., Shahinian A.H., Wang H., Park R., Conti P.S. (2010). Evaluation of copper-64 labeled AmBaSar conjugated cyclic RGD peptide for improved MicroPET imaging of integrin alphavbeta3 expression. Bioconjug Chem.
4 Haubner R., Beer A.J., Wang H., Chen X. (2010). Positron emission tomography tracers for imaging angiogenesis. Eur J Nucl Med Mol Imaging.
5 Cai H., Li Z., Huang C.W., Park R., Shahinian A.H., Conti P.S. (2010). An improved synthesis and biological evaluation of a new cage-like bifunctional chelator, 4-((8-amino-3,6,10,13,16,19-hexaazabicyclo[6.6.6]icosane-1-ylamino)methyl) benzoic acid, for 64Cu radiopharmaceuticals. Nucl Med Biol.